# N-(3-[^18^F]Fluoropropyl)-2β-carbomethoxy-3β-(4-iodophenyl)nortropane

Chemical name: | N-(3-[^18^F]Fluoropropyl)-2β-carbomethoxy-3β-(4-iodophenyl)nortropane
Abbreviated name: | [^18^F]FP-CIT, [^18^F]β-CIT-FP
Synonym: | 2-Carbomethoxy-8-(3-[^18^F]fluoropropyl)-3-(4-iodophenyl)tropane, N-ω-[^18^F]Fluoropropyl-2β-carbomethoxy-3β-(4-iodophenyl)tropane
Agent category: | Compound
Target: | Dopamine transporter
Target category: | Transporter
Method of detection: | Positron emission tomography, PET
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Non-Human Primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%5BAll%20Fields%5D%20AND%20%222-carbomethoxy-8-%283-fluoropropyl%29-3-%284-iodophenyl%29tropane%22%5BSubstance%20Name%5D)]

Dopamine, a neurotransmitter, plays an important role in the mediation of movement, cognition, and emotion. Parkinson’s disease (PD) is associated with a loss of dopamine-containing neurons in the striatum, resulting in a loss of dopamine transporters (DAT) in the presynaptic nerve terminals (1, 2). Reduction of DAT density is inversely correlated with the severity of motor dysfunction in PD patients. Several cocaine analogs were developed for the evaluation of DAT density in neurons of PD patients. Radiolabeled 2β-carboxymethoxy-3β-(4-iodophenyl)tropane (β-CIT) and N-(3-fluoropropyl)-2β-carbomethoxy-3β-(4-iodophenyl)nortropane (FP-CIT) have been used for brain imaging (3-6). Because of the short physical half-live of ^11^C- of ^11^C-labeled analogs, equilibrium conditions are difficult to achieve in positron emission tomography (PET) measurements. [^123^I]β-CIT was studied in single photon emission computed tomography (SPECT), which showed slow tracer uptake kinetics (7, 8). This led to the development of N-(3-[^18^F]fluoropropyl)-2β-carbomethoxy-3β-(4-iodophenyl)nortropane ([^18^F]FP-CIT) for PET brain imaging in PD patients (4).

### Related Resource Links:

- Chapters in MICAD (Dopamine transporter (http://www.ncbi.nlm.nih.gov/books?term=dopamine%20transporter%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (Dopamine transporter (http://www.ncbi.nlm.nih.gov/gene/6531))
- Articles in Online Mendelian Inheritance in Man (OMIM) (Dopamine transporter (http://www.ncbi.nlm.nih.gov/omim/126455))
- Clinical trials (FP-CIT (http://www.clinicaltrials.gov/ct2/results?term=FP-CIT))
- Drug information in FDA (FP-CIT (http://google2.fda.gov/search?q=FP-CIT&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=19&y=6))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%5BAll%20Fields%5D%20AND%20%222-carbomethoxy-8-%283-fluoropropyl%29-3-%284-iodophenyl%29tropane%22%5BSubstance%20Name%5D%20AND%20synthesis%5BAll%20Fields%5D)]

[^18^F]FP-CIT was synthesized by a nucleophilic fluorination of the mesylate precursor using the standard [^18^F] potassium Kryptofix complex. This method was automated to give a radiochemical yield of 1-2% (not decay corrected) in 80 min and a radiochemical purity of 98% (4). In another synthesis, [^18^F]fluoropropyl bromide was prepared by a nucleophilic fluorination of 1,3-dibromopropane with [^18^F] potassium Kryptofix complex. [^18^F]Fluoropropyl bromide was used to alkylate nor-CIT to form [^18^F]FP-CIT with a radiochemical yield of 2-4% and a radiochemical purity of 99%. The total synthesis time was about 90 min (6).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%5BAll%20Fields%5D%20AND%20%222-carbomethoxy-8-%283-fluoropropyl%29-3-%284-iodophenyl%29tropane%22%5BSubstance%20Name%5D%20AND%20in%20vitro)]

FP-CIT was reported to bind to both dopaminergic and serotonergic transporters in rat forebrain membrane homogenates (9). The transporter-binding affinity of FP-CIT was evaluated by competitive radioaffinity assays for DAT, serotonin, and norepinephrine with [^3^H]GBR 12935, [^3^H]paroxetine, and [^3^H]nisoxetine, respectively. Binding affinities (K_i_, nM) of FP-CIT at DAT, serotonin, and norepinephrine were 3.50, 0.11, and 63.0, respectively. FP-CIT showed lower DAT affinity than β-CIT for DAT and more selective affinity for the serotonin over DAT. Therefore, FP-CIT is useful as a tracer for DA neurons in the striatum and for serotonin neurons in the other brain areas.

## Animal Studies

### Rodent Studies

[PubMed] (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%5BAll%20Fields%5D%20AND%20%222-carbomethoxy-8-%283-fluoropropyl%29-3-%284-iodophenyl%29tropane%22%5BSubstance%20Name%5D%20AND%20rodentia)

No publication is currently available.

### Other Non-Primate Mammal Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2818f%5BAll%20Fields%5D%20AND%20cit%5BText%20Word%5D%20AND%20fp%5BAll%20Fields%5D%29%20AND%20animals%20NOT%20primates%20NOT%20rodentia)]

No publication is currently available.

### Non-Human Primate Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%5BAll%20Fields%5D%20AND%20%222-carbomethoxy-8-%283-fluoropropyl%29-3-%284-iodophenyl%29tropane%22%5BSubstance%20Name%5D%20AND%20monkeys%5BText%20Word%5D)]

[^18^F]FP-CIT PET studies were performed in cynomolgus monkeys (6). [^18^F]FP-CIT entered the brain rapidly. There was a high uptake in the striatum and much lower in the thalamus, neo-cortex, and cerebellum. The striatum-to-cerebellum ratio was about 5 at time of transient equilibrium, which occurred after 60-100 min. After pretreatment with GBR 12909, radioactivity in the striatum was markedly reduced, thus indicating specific [^18^F]FP-CIT binding to the dopamine transporters. The fraction of unchanged [^18^F]FP-CIT in monkey plasma determined by high-performance liquid chromatography (HPLC) was 10-15% after 25-140 min.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%5BAll%20Fields%5D%20AND%20%222-carbomethoxy-8-%283-fluoropropyl%29-3-%284-iodophenyl%29tropane%22%5BSubstance%20Name%5D%20AND%20human)]

Human dosimetry of [^18^F]FP-CIT was determined from blood samples and PET images in 12 human subjects after intravenous injection of [^18^F]FP-CIT, which was cleared rapidly from the blood to <10% in 15 min (10). Uptake in the lungs, heart, spleen, kidneys and liver peaked in 15-30 min and fell rapidly. The effective dose equivalent was 0.012 mSv/MBq (44 mrem/mCi). The organ that received the highest dose was the urinary bladder (0.059 mGy/MBq or 218 mrad/mCi), followed by the lungs (0.019 mGy/MBq or 70 mrad/mCi) and the liver (0.019 mGy/MBq or 70 mrad/mCi).

[^18^F]FP-CIT PET was first studied in one normal subject and one mildly affected PD patient (4). A higher uptake into striatal regions was observed in the normal brain than the PD brain. A reduction in putamenal uptake of 65% was observed in the PD patient. [^18^F]FP-CIT PET images of striatal uptake were more superior than those of [^123^I]FP-CIT SPECT. [^18^F]FP-CIT was cleared from the blood in 30 min. HPLC plasma analysis using [^18^F]FP-CIT indicated the presence of only one minor metabolite. A larger study was later performed using 15 early stage PD patients and 10 age-matched normal volunteers. Statistical parametric mapping was used to localize [^18^F]FP-CIT binding reduction in PD patients as compared to the normal volunteers. A reduction of 70% in ipsilateral putamen was observed in PD patients (11).

[^18^F]FP-CIT PET scan is a useful tool in clinical practice to support the diagnosis of PD and to differentiate between other pathological conditions. Moreover, [^18^F]FP-CIT PET could significantly impact treatment selection and follow-up of these patients.

## References

1 Carbon M., Ghilardi M.F., Feigin A., Fukuda M., Silvestri G., Mentis M.J., Ghez C., Moeller J.R., Eidelberg D. (2003). Learning networks in health and Parkinson's disease: reproducibility and treatment effects. Hum Brain Mapp.
2 Chesselet M.F., Delfs J.M. (1996). Basal ganglia and movement disorders: an update. Trends Neurosci.
3 Abi-Dargham A., Gandelman M.S., DeErausquin G.A., Zea-Ponce Y., Zoghbi S.S., Baldwin R.M., Laruelle M., Charney D.S., Hoffer P.B., Neumeyer J.L., Innis R.B. (1996). SPECT imaging of dopamine transporters in human brain with iodine-123-fluoroalkyl analogs of beta-CIT. J Nucl Med.
4 Chaly T., Dhawan V., Kazumata K., Antonini A., Margouleff C., Dahl J.R., Belakhlef A., Margouleff D., Yee A., Wang S., Tamagnan G., Neumeyer J.L., Eidelberg D. (1996). Radiosynthesis of [18F] N-3-fluoropropyl-2-beta-carbomethoxy-3-beta-(4-iodophenyl) nortropane and the first human study with positron emission tomography. Nucl Med Biol.
5 Kazumata K., Dhawan V., Chaly T., Antonini A., Margouleff C., Belakhlef A., Neumeyer J., Eidelberg D. (1998). Dopamine transporter imaging with fluorine-18-FPCIT and PET. J Nucl Med.
6 Lundkvist C., Halldin C., Ginovart N., Swahn C.G., Farde L. (1997). [18F] beta-CIT-FP is superior to [11C] beta-CIT-FP for quantitation of the dopamine transporter. Nucl Med Biol.
7 Ishikawa T., Dhawan V., Kazumata K., Chaly T., Mandel F., Neumeyer J., Margouleff C., Babchyck B., Zanzi I., Eidelberg D. (1996). Comparative nigrostriatal dopaminergic imaging with iodine-123-beta CIT-FP/SPECT and fluorine-18-FDOPA/PET. J Nucl Med.
8 Laruelle M., Wallace E., Seibyl J.P., Baldwin R.M., Zea-Ponce Y., Zoghbi S.S., Neumeyer J.L., Charney D.S., Hoffer P.B., Innis R.B. (1994). Graphical, kinetic, and equilibrium analyses of in vivo [123I] beta-CIT binding to dopamine transporters in healthy human subjects. J Cereb Blood Flow Metab.
9 Neumeyer J.L., Tamagnan G., Wang S., Gao Y., Milius R.A., Kula N.S., Baldessarini R.J. (1996). N-substituted analogs of 2 beta-carbomethoxy-3 beta- (4'-iodophenyl)tropane (beta-CIT) with selective affinity to dopamine or serotonin transporters in rat forebrain. J Med Chem.
10 Robeson W., Dhawan V., Belakhlef A., Ma Y., Pillai V., Chaly T., Margouleff C., Bjelke D., Eidelberg D. (2003). Dosimetry of the dopamine transporter radioligand 18F-FPCIT in human subjects. J Nucl Med.
11 Ma Y., Dhawan V., Mentis M., Chaly T., Spetsieris P.G., Eidelberg D. (2002). Parametric mapping of [18F]FPCIT binding in early stage Parkinson's disease: a PET study. Synapse.